# ^68^Ga-Labeled β-aminoalanine, γ-aminohomoalanine, and ε-aminolysine conjugates of 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid

Chemical name: | ^68^Ga-labeled β-aminoalanine, γ-aminohomoalanine, and ε-aminolysine conjugates of 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid | [image]
Abbreviated name: | ^68^Ga-2a-c | [image]
Synonym: | ^68^Ga-2a, ^68^Ga-2b, ^68^Ga-2c | [image]
Agent Category: | Others (amino acid) | [image]
Target: | Amino acid transporters | [image]
Target Category: | Transporters | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | Gallium-68 (^68^Ga) | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of 2a-c (n = 1, β-aminoalanine; n = 2, γ-aminohomoalanine; and n = 4, ε-aminolysine) by Shetty et al. (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=amino%20acid%20and%20imaging%20and%20amino%20acid%20transporters)]

The ^68^Ga-labeled â-aminoalanine, ã-aminohomoalanine, and å-aminolysine conjugates of 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (DOTA), abbreviated as ^68^Ga-2a, ^68^Ga-2b, and ^68^Ga-2c, respectively, were synthesized by Shetty et al. for positron emission tomography (PET) of tumors (1).

Radiolabeled amino acids represent a diverse class of tracers that target the increased amino acid transport in cancer cells (2, 3). To date, >20 distinct amino acid transporters have been identified in mammalian cells, and these transporters differ in terms of substrate specificity, tissue expression patterns, sodium and other ion dependence, pH sensitivity, and transport mechanism (4, 5). Because of increased demand for amino acids in malignant cells, some transporters have been shown to be overexpressed in different types of tumors, and the process of amino acid transport is relatively fast (1, 2, 6). These features make tumor imaging with amino acid tracers possible within 20 min. Indeed, there is growing evidence that radiolabeled amino acids have the potential to overcome some of the limitations of 2-deoxy-2-[^18^F]fluoro-D-glucose ([^18^F]FDG) in tumor imaging, especially in the imaging of primary and recurrent brain tumors, neuroendocrine tumors, and prostate cancers (2, 3, 7). Different studies also showed that radiotracers that target different amino acid transporters exhibit different imaging properties that may provide unique biological information of tumors (1, 2, 8).

The first group of widely investigated amino acids is the analogs of phenylalanine and tyrosine (2, 3). Because of their bulky neutral side chains, these natural amino acids are the substrates of system L transporters and have been proven to be useful for tumor imaging, particularly for brain tumors. The limitation common to most of the natural amino acids is the susceptibility to in vivo metabolism, which decreases tumor specificity and complicates kinetic analysis. Because none of the natural amino acids contain fluorine or iodine, labeling with fluorine-18 or iodine-123 and retaining key biochemical properties are also challenging. These shortcomings associated with natural amino acids can be partially overcome by using non-natural amino acids. Typically, non-natural amino acids are neither metabolized nor readily incorporated into protein in vivo (1-3). One group of non-natural amino acids is á,á-dialkyl amino acids, which are generated by substituting the á-carbon hydrogen of natural amino acids with a methyl group or other alkyl chains. These amino acids are primarily the substrates of system A transporters. The second group is alicyclic amino acids, which are á,á-dialkyl amino acids with side chains bonded covalently to each other to form a cyclic ring. These amino acids are the substrates of system L transporters. The third group is the non-natural proline derivatives, which exhibit different transport selectivity. One challenge in developing amino acid radiotracers is to overcome the low selectivity and the decreased recognition after radiolabeling to specific transporters (2, 3, 8). Another challenge is the low uptake of amino acid agents in tumors, which leads to less sensitivity for tumor detection than with [^18^F]FDG (7).

Shetty et al. synthesized a group of ^68^Ga-labled alanine and lysine derivatives of DOTA, 1,4,7-triazacyclononane-1,4,7-triacetic acid (NOTA), 1,4,7,10-tetraazacyclododecane-1,7-diacetic acid (DO2A), and 1,4,7,10-tetraazacyclododecane-1,4,7,-triacetic acid (DO3A) (1, 8). The four bifunctional chelating agents have similar sizes, but they differ in the net charges and stability because of the different numbers of pendent carboxylate arms. The amino acids have been conjugated to one of the carboxylate arms, and the nitrogen atoms in the heterocyclic ring are presumed to coordinate with metals to form chelates. Biodistribution studies and PET imaging indicate the structure–activity relationship of the amino acid derivatives, and the selective uptakes of these compounds by different cancer tissues might provide an insight on the different modes of amino acid uptake by cancer cells (1, 8).

This chapter summarizes the data obtained with ^68^Ga-labeled DOTA derivatives: ^68^Ga-2a (^68^Ga-DOTA-â-aminoalanine), ^68^Ga-2b (^68^Ga-DOTA-ã-aminohomoalanine), and ^68^Ga-2c (^68^Ga-DOTA-å-aminolysine). These DOTA derivatives were comparatively analyzed with the corresponding NOTA derivatives (^68^Ga-1a, ^68^Ga-1b, and ^68^Ga-1c, respectively) (1).

### Related Resource Links:

Amino acid transporter-targeted imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=amino+acid+transporter+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Amino acid transporter articles in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/omim/?term=amino+acid+transporter)

Amino acid transporter related clinical trials in ClinicalTrials.gov (http://clinicaltrials.gov/ct2/results?term=amino+acid+transporter)

Amino acid transporter related bioassays in PubChem BioAssay (http://www.ncbi.nlm.nih.gov/pcassay/?term=amino+acid+transporter)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20926300)]

The protected â-amino-L-alanine was synthesized from N-tert-butyl-L-serine methyl ester. Conjugation of DOTA with protected â-amino-L-alanine was performed in aqueous solution using 1-ethyl-3-[3-(dimethylamino)propyl]carbodiimide hydrochloride as a coupling reagent to obtain the alanine conjugate. Hydrolysis of the protected esters using LiOH, followed by hydrochloric acid, resulted in the formation of compound 2a (DOTA-â-aminoalanine) as a hydrochloride salt.

The ã-amino-L-homoalanine was purchased, and the å-aminolysine was synthesized from N^á^-boc-N^å^-benzyloxycarbonyl-lysine by tert-butyl esterification and subsequent deprotection. Conjugation of ã-amino-L-homoalanine and å-aminolysine with DOTA was performed separately with N,N'-dicyclohexylcarbodiimide as a coupling agent and pyridine as a base. Further hydrolysis and deprotection resulted in the formation of compound 2b (DOTA-ã-aminohomoalanine) and compound 2c (DOTA-å-aminolysine), respectively. All final products were purified (1).

The DOTA and NOTA derivatives were labeled with ^68^Ga either in a boiling water bath or at room temperature (1). The chelating agents, DOTA and NOTA, were also labeled with ^68^Ga as controls for the in vitro protein binding and cell uptake studies. The labeling efficiency was >95% for all agents, and no free ^68^Ga was found after purification. The specific activities of the purified agents were in the range 1.94–9.21 GBq/ìmol (52.43–248.92 mCi/µmol). Stability studies at room temperature confirmed the stability of all agents for >4 h.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20926300)]

Shetty et al. performed protein binding studies by incubating the agents with human serum at 37°C for 10 min and 1 h, respectively (1). ^68^Ga-2c showed the lowest level of protein binding (2.44% at 10 min and 5.57% at 1 h), followed by ^68^Ga-2b (6.40% at 10 min and 6.60% at 1 h) and ^68^Ga-2a (9.87% at 10 min and 9.81% at 1 h). In comparison with the corresponding NOTA derivatives, all DOTA derivatives had higher levels of serum protein binding. Only the DOTA derivatives showed significant increases in protein binding over time. Of all NOTA and DOTA derivatives, ^68^Ga-1b showed the lowest level of protein binding (1.71% at 10 min and 1.44% at 1 h) and ^68^Ga-2a showed the highest level of binding (1). NOTA is known to form more stable chelate with ^68^Ga than DOTA, and thus, ^68^Ga might be transchelated to serum proteins such as transferrin from the less stable chelates of DOTA and its derivatives.

Cell uptake studies after incubation of the cells with each agent showed that all three agents had significantly higher uptakes than the control compounds (^68^Ga-NOTA and ^68^Ga-DOTA) in both Hep3B (a human hepatoma cell line) and CT-26 (a mouse colon cancer cell line) cells (1). Of the three agents, ^68^Ga-2a had the highest uptake in Hep3B cells, while ^68^Ga-2b had the highest uptake in CT-26 cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20926300)]

The biodistribution of ^68^Ga-2a, ^68^Ga-2b, and ^68^Ga-2c (10 ìCi/0.1 ml (0.37 MBq/0.1 ml)) was investigated after tail vein injection in mice bearing human colon cancer CT-26 xenografts (n = 4 mice/time point for each agent) (1). Mice were euthanized at different times (10, 30, 60, and 120 min) after injection, and counts were obtained with a ã-scintillation counter. Tumor uptakes for all three agents were higher than those for most organs, except for the kidneys. Tumor/blood ratios were similar for all agents up to 60 min after injection but differed at 120 min. The tumor/blood ratios for ^68^Ga-2a, ^68^Ga-2b, and ^68^Ga-2c were 0.72, 0.9, and 0.96, respectively, at 60 min after injection, and were 1.02, 1.41, and 1.73, respectively, at 120 min after injection. Tumor/muscle ratios were different among the agents. The highest tumor/muscle ratio was achieved by ^68^Ga-2a (2.48), followed by ^68^Ga-2b (1.65) and ^68^Ga-2c (1.51) at 30 min after injection.

PET imaging in mice bearing human colon cancer CT-26 xenografts was performed at 30 min after injection of the agents (0.6–0.8 mCi (22.2–29.6 MBq)) through the tail vein (1). High levels of kidney and bladder activity were observed for all agents, indicating rapid renal excretion. Tumor uptakes were visualized by PET with all three agents (^68^Ga-2a, ^68^Ga-2b, and ^68^Ga-2c), but ^68^Ga-2a demonstrated the highest tumor/muscle ratio (5.9).

In comparison between DOTA and NOTA derivatives, all agents showed fast renal excretion and blood clearance, low nonspecific uptake in normal organs except for kidneys, and relatively high uptake in tumor tissues (1). In biodistribution studies, the tumor/blood ratios for NOTA-amino acid derivatives were higher than those for DOTA-amino acid derivatives at 2 h, although the ratios were similar for all six agents at 30 min after injection, which might be related to the higher serum protein binding by DOTA derivatives. In PET imaging, ^68^Ga-1b demonstrated the highest tumor/muscle ratio (12.3), followed by ^68^Ga-2a (5.9) and ^68^Ga-2b (4.3). These results suggest that ^68^Ga-1b is more favorable than others for use in PET imaging of tumors (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Shetty D., Jeong J.M., Ju C.H., Kim Y.J., Lee J.Y., Lee Y.S., Lee D.S., Chung J.K., Lee M.C. (2010). Synthesis and evaluation of macrocyclic amino acid derivatives for tumor imaging by gallium-68 positron emission tomography. Bioorg Med Chem.
2 McConathy, J., W. Yu, N. Jarkas, W. Seo, D.M. Schuster, and M.M. Goodman, Radiohalogenated nonnatural amino acids as PET and SPECT tumor imaging agents. Med Res Rev, 2011
3 Laverman P., Boerman O.C., Corstens F.H., Oyen W.J. (2002). Fluorinated amino acids for tumour imaging with positron emission tomography. Eur J Nucl Med Mol Imaging.
4 Ganapathy V., Thangaraju M., Prasad P.D. (2009). Nutrient transporters in cancer: relevance to Warburg hypothesis and beyond. Pharmacol Ther.
5 Goberdhan D.C. (2010). Intracellular amino acid sensing and mTORC1-regulated growth: new ways to block an old target?. Curr Opin Investig Drugs.
6 Fuchs B.C., Bode B.P. (2005). Amino acid transporters ASCT2 and LAT1 in cancer: partners in crime?. Semin Cancer Biol.
7 la Fougere C., Suchorska B., Bartenstein P., Kreth F.W., Tonn J.C. (2011). Molecular imaging of gliomas with PET: Opportunities and limitations. Neuro Oncol.
8 Shetty D., Jeong J.M., Ju C.H., Lee Y.S., Jeong S.Y., Choi J.Y., Yang B.Y., Lee D.S., Chung J.K., Lee M.C. (2010). Synthesis of novel 68Ga-labeled amino acid derivatives for positron emission tomography of cancer cells. Nucl Med Biol.